# Ovarian cancer antigen 183B2 monoclonal antibody conjugated to ultrasmall superparamagnetic iron oxide nanoparticles

Chemical name: | Ovarian cancer antigen 183B2 monoclonal antibody conjugated to ultrasmall superparamagnetic iron oxide nanoparticles
Abbreviated name: | OCMab183B2-USPIO
Synonym:
Agent category: | Antibody
Target: | OC183B2
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20OC183B2)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules, which comprise ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or another polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO nanoparticles, standard SPIO nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (1).

USPIO is composed of iron nanoparticles with diameters of 4–6 nm, and the hydrodynamic diameters with dextran or polyethylene glycol (PEG) coating are 20–50 nm. USPIO nanoparticles have a long plasma half-life because of their small size. The blood pool half-life is calculated to be ~24 h in humans (2) and 2 h in mice (3). Because of its long blood half-life, USPIO can be used as a blood pool agent during the early phase of intravenous administration (4). In the late phase, USPIO is suitable for the evaluation of RES in the body, particularly in the lymph nodes (5). Various ligands and antibody-conjugated USPIO nanoparticles have been studied for in vivo targeted MRI in small animals (6, 7). Qian et al. (8) have identified ovarian cancer antigen OC183B2 on SKOV-3 human epithelial ovarian carcinoma cells and obtained its monoclonal antibody, OCMab183B2. Quan et al. (9) coupled OCMab183B2 to USPIO nanoparticles for in vivo MRI of ovarian cancer in mice.

### Related Resource Links:

- Chapters in MICAD (USPIO (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=USPIO+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Clinical trials (USPIO (http://www.clinicaltrials.gov/ct2/results?term=USPIO))
- Drug information in FDA (SPIO (http://google2.fda.gov/search?q=spio&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20OC183B2%20and%20synthesis)]

A solution of Fe(acac)_3_ and HOOC-polyethylene glycol (PEG)-COOH (2 kDa) in 2-pyrrolidone was incubated for 30 min at 200°C and then for 90 min at 240°C (9). The resulting nanoparticles have an average hydrodynamic diameter of ~40 nm. OCMab183B2 was coupled to USPIO via an ethyl-3-(dimethylaminopropyl)carbodiimide-mediation reaction between the primary amine groups of OCMab183B2 and the monocarboxylic group of PEG of the USPIO nanoparticles. Control mIgG-USPIO nanoparticles were also prepared similarly. The number of antibody molecules per USPIO nanoparticle was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20OC183B2%20and%20in%20vitro)]

Quan et al. (9) performed in vitro binding studies of OCMab183B2-USPIO, mIgG-USPIO, and USPIO nanoparticles (20 µg Fe/ml) in cultured SKOV-3 cells with T2-weighted MRI (3 T). OCMab183B2-USPIO exhibited a decrease in T2-weighted MRI images in comparison to mIgG-USPIO and USPIO. Immunocytochemical staining of the SKOV-3 cells treated with OCMab183B2-USPIO and USPIO showed that 96% of SKOV-3 cells were labeled with OCMab183B2-USPIO after 24 h of incubation, whereas only 63% of SKOV-3 cells were labeled with USPIO. OCMab183B2-USPIO showed little cytotoxic effect on SKOV-3 cells up to 120 µg Fe/ml for 20 h. No blocking experiment was performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20OC183B2%20and%20rodentia)]

Quan et al. (9) performed T2-weighted MRI (3 T) in mice bearing SKOV-3 xenografts with OCMab183B2-USPIO (n = 12) and mIgG-USPIO (n = 6) at 5 min to 48 h after injection. Injection of OCMab183B2-USPIO resulted in a decrease in MRI contrast, which reached a maximal 38.5% decrease in T2 relaxation time in the tumors at 24 h after injection. T2 relaxation time of mIgG-USPIO reached the maximal 15.4% decrease in T2 relaxation time in the tumors at 2 h after injection. T2 relaxation times in both tumors were similar at 48 h. At 24 h, there was a significant (P < 0.02) difference between the T2 relaxation times exhibited by OCMab183B2-USPIO (70.19 ± 17.20) and mIgG-USPIO (106.94 ± 12.53). Histochemical staining of tumor sections with Prussian blue at 48 h after injection showed the presence of iron inside the tumor cells from mice injected with OCMab183B2-USPIO but not in tumor cells from mice injected with mIgG-USPIO. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20OC183B2%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20OC183B2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20OC183B2%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
3 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
4 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
5 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
6 Boutry S., Laurent S., Elst L.V., Muller R.N. (2006). Specific E-selectin targeting with a superparamagnetic MRI contrast agent. Contrast Media Mol Imaging.
7 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
8 Qian H.N., Feng J., Cui H., Fu T.Y., Wei P., Fu Z.Y. (1989). Generation and characterization of three monoclonal antibodies to human ovarian epithelial adenocarcinomas. Chin Med J (Engl).
9 Quan G., Du X., Huo T., Li X., Wei Z., Cui H., Chang X., Cheng Y., Ye X., Cheng H. (2010). Targeted molecular imaging of antigen OC183B2 in ovarian cancers using MR molecular probes. Acad Radiol.